# [^177^Lu]-Labeled 2-(4-isothiocyanatobenzyl)-6-methyldiethylene-triaminepentaacetic acid (1B4M-DTPA) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII)

Chemical name: | [^177^Lu]-Labeled 2-(4-isothiocyanatobenzyl)-6-methyldiethylene-triaminepentaacetic acid (1B4M-DTPA) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII)
Abbreviated name: | [^177^Lu]1B4M-DTPA-L8A4
Synonym:
Agent Category: | Monoclonal antibody
Target: | Epidermal growth factor receptor variant III (EGFRvIII)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography; gamma planar imaging
Source of signal / contrast: | ^177^Lu
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ch806&cmd=DetailsSearch)]

The biological characteristics, activating ligands, functions, and signal transduction pathways of the various transmembrane epidermal growth factor receptors (EGFRs) are described elsewhere (1-3). The EGFRs are known to regulate the growth, survival, differentiation, and migration of cells through the activation of an associated intracellular tyrosine kinase (TK) signaling pathway, and they are overexpressed in many malignant epithelial tumors (2, 3). Overexpression of the EGFR in tumors has been attributed to cellular amplification of the receptor gene, and this phenomenon may result in the production of a mutated receptor in the cell (2, 4). In addition, overexpression of the EGFR in tumors usually indicates a poor clinical prognosis for a cancer patient (4). The most common mutation observed in the receptor is the deletion of an extracellular domain segment of the EGFR, including the ligand-binding region, and this generates a variant known as EGFRvIII or de2-7 EGFR (2, 4). The generation, structure, functions, and role of EGFRvIII in tumor malignancy was reviewed by Gan et al. (5). Although EGFRvIII is nonresponsive to a ligand due to the absence of a ligand-binding site, it is constitutively active with a constantly operating downstream TK signal transduction pathway that appears to promote the development of a neoplastic phenotype, particularly for glioblastoma and to some extent for other cancers such as those of the prostate and the breast (2, 6).

Because the EGFR promotes and helps maintain transformed cells, several anti-EGFR antibodies (http://google2.fda.gov/search?q=anti-EGFR+antibodies+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=6) that inhibit the activity of this receptor and small molecule drugs (http://google2.fda.gov/search?q=EGFR+Tyrosine+kinase+inhibitor&spell=1&client=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&ie=UTF-8&site=FDAgov&access=p) that block the downstream TK signaling pathway were developed and have been approved by the United States Food and Drug Administration for the treatment of certain cancers (2). The antibodies are designed to target the extracellular domain of the receptor, block ligand binding, and inhibit activation of the TK signal transduction pathway, which leads to downregulation of the EGFR on the cell surface. However, because EGFRvIII lacks the ligand-binding region on the extracellular domain, these antibodies cannot obstruct the constitutive mutant receptor activity (2). Hence, a monoclonal antibody (mAb), designated mAb806 and specifically targets the EGFRvIII, was generated and has been characterized in preclinical studies (7, 8). Subsequently, a chimeric form of the mAb (chAb), designated ch806, was developed and evaluated in a phase I clinical trial involving patients with cancerous tumors that overexpressed the EGFRvIII. Results from this trial indicated that ch806 can be a suitable biotherapeutic agent to treat cancers (4). Various studies performed with mAb806 or ch806 are described in separate chapters of MICAD (http://www.ncbi.nlm.nih.gov/books/?term=ch806%20AND%20micad%5Bbook%5D).

Studies are also in progress with another anti-EGFRvIII mAb, L8A4, to develop a radioimmunotherapeutic (RIT) agent for the treatment of cancer (9, 10). In a recent study, the use of acyclic ([(R)-2-amino-3-(4-isothiocyanatophenyl)propyl]-trans-(S,S)-cyclohexane-1,2-diamine-pentaacetic acid (CHX-A''-DTPA) and 2-(4-isothiocyanatobenzyl)-6-methyldiethylene-triaminepentaacetic acid (1B4M-DTPA) as well as the macrocyclic ligands (S)-2-(4-isothiocyanatobenzyl)-1,4,7,10-tetraazacyclododecane-tetraacetic acid (C-DOTA) and α-(5-isothiocyanato-2-methoxyphenyl)-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (MeO-DOTA) was evaluated for the labeling of L8A4 with ^177^Lu, which was considered suitable to generate an RIT agent against cancer (10). The characteristics of the various ^177^Lu-labeled conjugates of L8A4 ([^177^Lu]-CHX-A''-DTPA-L8A4, [^177^Lu]-1B4M-DTPA-L8A4, [^177^Lu]-C-DOTA-L8A4, and [^177^Lu]-MeO-DOTA-L8A4) were compared to the characteristics of L8A4 labeled with N-succinimidyl 4-guanidinomethyl-3-[^125^I]iodobenzoate ([^125^I]SGMIB-L8A4) under in vitro (9) and in vivo (10) conditions.

This chapter describes results obtained from the in vitro and the biodistribution studies performed with[^177^Lu]-1B4M-DTPA-L8A4 in athymic mice bearing subcutaneous U87MG.∆EGFR cell glioma xenograft tumors. Results obtained with [^125^I]SGMIB-L8A4, [^177^Lu]-CHX-A''-DTPA-L8A4 , [^177^Lu]-C-DOTA-L8A4, and [^177^Lu]-MeO-DOTA-L8A4 are presented in separate chapters of MICAD (www.micad.nih.gov) (11-14).

### Other Sources of Information

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_005228.3) of human EGFR variant 1

EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim/131550) (Online Mendelian Inheritance in Man)

EGFR signaling pathways (http://pid.nci.nih.gov/search/pathway_landing.shtml?pathway_id=200086&source=NATURE&what=graphic&jpg=on) (NCI-Nature Pathways Interaction Database)

Anti-EGFR antibodies (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-EGFR%20antibodies&cmd=DetailsSearch) in PubMed

EGFR tyrosine kinase inhibitors (http://www.ncbi.nlm.nih.gov/pubmed?term=egfr%20tyrosine%20kinase%20inhibitors&cmd=DetailsSearch) in PubMed

Chapters on anti-EGFR antibodies (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad) in MICAD

Other chapters on anti-EGFRvIII antibodies (http://www.ncbi.nlm.nih.gov/books/?term=EGFRvIII%20AND%20micad%5Bbook%5D) in MICAD

Clinical trials (http://clinicaltrials.gov/ct2/results?term=EGFRvIII+) with EGFRvIII as a target

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Synthesis%20of%20L8A4%20antibody&cmd=DetailsSearch)]

The preparation, purification, characterization, conjugation of L8A4 with 1B4M-DTPA or CHX-A''-DTPA, and the radiolabeling of 1B4M-DTPA-L8A4 and CHX-A''-DTPA-L8A4 with ^177^Lu are discussed by Hens et al. (10). The production of [^125^I]SGMIB-L8A4 (labeled with N-succinimidyl 4-guanidinomethyl-3-[^125^I]iodobenzoate ([^125^I]SGMIB)) is also described by Hens et al. (10). The radiochemical yield (RCY) of [^177^Lu]-1B4M-DTPA-L8A4 and [^177^Lu]-CHX-A''-DTPA-L8A4 was 86% and 76%, respectively (9). The RCY of [^125^I]SGMIB-L8A4 and the purity of the three labeled mAbs was not reported. The specific activity (SA) of [^177^Lu]-1B4M-DTPA-L8A4 and [^177^Lu]-CHX-A''-DTPA-L8A4 was reported to be 0.066MBq/6.6 pmol (1.8 μCi/6.6 pmol) and 0.092 MBq/6.6 pmol (2.5 μCi/6.6 pmol), respectively. The SA of of [^125^I]SGMIB-L8A4 varied from 0.111–0.185 MBq/6.6 pmol (3–5 μCi/6.6 pmol) to 0.026–0.118 MBq/6.6 pmol (0.7–3.2 μCi/6.6 pmol). The three labeled mAbs were shown to elute as a single peak with non-labeled L8A4 and had a similar retention time as the native mAb when analyzed with a size-exclusion column using high performance liquid chromatography. Each mAb molecule was determined to bear 1.1 and 0.3 moieties of 1B4M-DTPA and CHX-A''-DTPA, respectively (9, 10).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20in%20vitro%20studies&cmd=DetailsSearch)]

Using a magnetic bead assay, the immunoreactive fractions of [^177^Lu]-1B4M-DTPA-L8A4 and [^177^Lu]-CHX-A''-DTPA-L8A4 were determined to be76% and 60%, respectively, compared to between 60% to 71% for [^125^I]SGMIB-L8A4 (9). A cell internalization assay with U87MG.∆EGFR cells showed that internalization of both [^177^Lu]-1B4M-DTPA-L8A4 and [^177^Lu]-CHX-A''-DTPA-L8A4 continued to increase for at least 24 h (was ~35% at this time point for both). In contrast internalization of the ^125^I-labeled mAb peaked to ~10% of the original cell-bound radioactivity at 1 h after exposure and was reduced to ~1% of the original value by 24 h after exposure.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^177^Lu]-1B4M-DTPA-L8A4 and [^177^Lu]-CHX-A''-DTPA-L8A4 was compared it to that of [^125^I]SGMIB-L8A4 in athymic mice (n = 5 animals/group) bearing subcutaneous U87MG.∆EGFR cell glioma xenograft tumors as described by Hens et al. (10). Animals in the different groups were co-injected (route of injection not reported) with either [^177^Lu]-1B4M-DTPA-L8A4 and [^125^I]SGMIB-L8A4 or [^177^Lu]-CHX-A''-DTPA-L8A4 and [^125^I]SGMIB-L8A4. The rodents were euthanized at 1, 4, and 8 days postinjection (p.i.) of the labeled mAbs and all major organs were harvested from the animals. Radioactivity incorporated in the various organs was counted using a dual-channel automated gamma counter and the data was presented as percent of injected dose per gram tissue (% ID/g).

With [^177^Lu]-1B4M-DTPA-L8A4 the amount of radioactivity in the blood was 19.78 ± 2.94% ID/g at 1 day p.i. and this was reduced to 1.35 ± 0.94% ID/g by 8 days p.i. At 1 day p.i., the liver, kidneys, spleen, lungs and bone exhibited an accumulation of between 8.36 ± 0.74% ID/g (liver) and 3.58 ± 1.44% ID/g (bone) and the by 8 days p.i. amount of label in all these organs, except the bone, decreased to between 0.93 ± 0.45% ID/g (lungs) and 4.16 ± 0.54% ID/g (Liver) (10). During this period the incorporation of radioactivity in the bone decreased from 3.58 ± 1.44% ID/g at 1 day p.i. to 1.82 ± 0.52% ID/g at 8 days p.i. The amount of tracer accumulated in the muscles was 1.64 ± 0.08% Id/g at 1 day p.i. and was reduced to 0.30 ± 0.07% ID/g by 8 days p.i. The amount of radioactivity accumulated in the tumor was 31.58 ± 6.60% ID/g at 1 day p.i. and decreased to 15.27 ± 5.16% ID/g by 8 days p.i. The tumor/normal tissue ratios for liver, kidneys, spleen, brain, and bone were reported to be approximately 3.8, 4, 4, 55, and 10, respectively, at 1 day p.i. and approximately 3.8, 6, 4, 200 and 8, respectively at 8 days p.i.

With [^177^Lu]-CHX-A''-DTPA-L8A4 the amount of radioactivity in the blood was 15.18 ± 3.30% ID/g at 1 day p.i. and this was was reduced to 0.99 ± 0.71% ID/g by 8 days p.i. At 1 day p.i., the liver, kidneys, spleen, lungs and bone exhibited accumulation of between 8.53 ± 1.86% ID/g (liver) and 5.98 ± 1.86% ID/g (spleen) and the by 8 days p.i. amount of label in all these organs, except the bone, decreased to between 0.56 ± 0.23% ID/g (lungs) and 4.45 ± 0.87% ID/g (Liver). During this period the incorporation of radioactivity in the bone increased from 5.95 ± 1.27% ID/g at 1 day p.i. to 7.56 ± 1.88% ID/g at 8 days p.i. This phenomenon was attributed to the bone seeking character of ^177^Lu indicating that [^177^Lu]-CHX-A''-DTPA-L8A4 may not be suitable detection agent for EGFRvIII expressing tumors. The amount of tracer accumulated in the muscles was 1.30 ± 0.44% Id/g at 1 day p.i. and was reduced to 0.19 ± 0.05% ID/g by 8 days p.i. The amount of radioactivity accumulated in the tumor was 36.28 ± 6.60% ID/g at 1 day p.i. and decreased to 8.67 ± 3.42% ID/g by 8 days p.i. The tumor/normal tissue ratios for liver, kidneys, spleen, brain, and bone were reported to be approximately 4, 6, 4, 95, and 6, respectively, at 1 day p.i. and approximately 2, 5, 2, 200 and 2, respectively at 8 days p.i.

With [^125^I]SGMIB-L8A4 the amount of radioactivity in the blood at 1 day p.i. was 18.78 ± 2.24% ID/g and decreased to 1.29 ± 0.87% ID/g by 8 days p.i. At 1 day p.i., the liver, kidneys, spleen, and lungs exhibited accumulation between 5% and 7% ID/g and the amount of label in all these organs decreased to ~0.5% ID/g by 8 days p.i. The amount of tracer accumulated in the muscles and bones was ~1.5 and ~3.5% ID/g, respectively, at 1 day p.i.; by 8 days p.i., accumulation decreased to ~0.15% ID/g and ~0.33% ID/g, respectively, in these tissues. The tumor had a radioactivity accumulation of 21.64 ± 4.53% ID/g at 1 day p.i., which decreased to 2.86 ± 0.98% ID/g by 8 days p.i. The tumor/normal tissue ratios for liver, kidneys, spleen, brain, and bone were reported to be approximately 6, 8, 6, 60, and 10, respectively, at 1 day p.i. and approximately 7, 8, 7, 60 and 6, respectively, at 8 days p.i.

Table 1: Summary of tumor/normal tissue radioactivity uptake ratios for various organs obtained with [^125^I]SGMIB-L8A4, [^177^Lu]1B4M-DTPA-L8A4 and [^177^Lu]CHX-A”-DTPA-L8A4. Data obtained from Figure 5 in Hens et al. (10).

Conjugated mAb | Liver | | Kidney | | Spleen | | Brain | | Bone
Conjugated mAb | Time after labeled mAb injection
Conjugated mAb | 1 day | 8 days | 1 day | 8 days | 1 day | 8 days | 1 day | 8 days | 1 day | 8 days
Conjugated mAb | Tumor-to-normal tissue ratio
[ ^ 125 ^ I]SGMIB-L8A4 | 6 | 7 | 8 | 8 | 6 | 7 | 60 | 60 | 10 | 6
[ ^ 177 ^ Lu]1B4M-DTPA-L8A4 | 3.8 | 3.8 | 4 | 6 | 4 | 4 | 55 | 200 | 10 | 8
[ ^ 177 ^ Lu]CHX-A”-DTPA-L8A4 | 4 | 2 | 6 | 5 | 4 | 2 | 95 | 200 | 6 | 2

Based on the results presented in Table 1, [^177^Lu]1B4M-DTPA-L8A4 appear to be superior to [^177^Lu]-CHX-A''-DTPA-L8A4 and [^125^I]SGMIB-L8A4 for the detection of EGFRvIII overexpressing tumors in rodents because it showed a lower incorporation of radioactivity in the bones and maintained the higher tumor-to-normal tissue ratios even at 8 days p.i (10).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

These studies were supported by National Institutes of Health grants NS20023 and CA42324.

## References

1 Hasselbalch B., Lassen U., Poulsen H.S., Stockhausen M.T. (2010). Cetuximab insufficiently inhibits glioma cell growth due to persistent EGFR downstream signaling. Cancer Invest.
2 Pines G., Kostler W.J., Yarden Y. (2010). Oncogenic mutant forms of EGFR: lessons in signal transduction and targets for cancer therapy. FEBS Lett.
3 Spector N.L., Blackwell K.L. (2009). Understanding the mechanisms behind trastuzumab therapy for human epidermal growth factor receptor 2-positive breast cancer. J Clin Oncol.
4 Scott A.M., Lee F.T., Tebbutt N., Herbertson R., Gill S.S., Liu Z., Skrinos E., Murone C., Saunder T.H., Chappell B., Papenfuss A.T., Poon A.M., Hopkins W., Smyth F.E., MacGregor D., Cher L.M., Jungbluth A.A., Ritter G., Brechbiel M.W., Murphy R., Burgess A.W., Hoffman E.W., Johns T.G., Old L.J. (2007). A phase I clinical trial with monoclonal antibody ch806 targeting transitional state and mutant epidermal growth factor receptors. Proc Natl Acad Sci U S A.
5 Gan H.K., Kaye A.H., Luwor R.B. (2009). The EGFRvIII variant in glioblastoma multiforme. J Clin Neurosci.
6 Lee F.T., O'Keefe G.J., Gan H.K., Mountain A.J., Jones G.R., Saunder T.H., Sagona J., Rigopoulos A., Smyth F.E., Johns T.G., Govindan S.V., Goldenberg D.M., Old L.J., Scott A.M. (2010). Immuno-PET quantitation of de2-7 epidermal growth factor receptor expression in glioma using 124I-IMP-R4-labeled antibody ch806. J Nucl Med.
7 Jungbluth A.A., Stockert E., Huang H.J., Collins V.P., Coplan K., Iversen K., Kolb D., Johns T.J., Scott A.M., Gullick W.J., Ritter G., Cohen L., Scanlan M.J., Cavenee W.K., Old L.J. (2003). A monoclonal antibody recognizing human cancers with amplification/overexpression of the human epidermal growth factor receptor. Proc Natl Acad Sci U S A.
8 Perera R.M., Zoncu R., Johns T.G., Pypaert M., Lee F.T., Mellman I., Old L.J., Toomre D.K., Scott A.M. (2007). Internalization, intracellular trafficking, and biodistribution of monoclonal antibody 806: a novel anti-epidermal growth factor receptor antibody. Neoplasia.
9 Hens M., Vaidyanathan G., Welsh P., Zalutsky M.R. (2009). Labeling internalizing anti-epidermal growth factor receptor variant III monoclonal antibody with (177)Lu: in vitro comparison of acyclic and macrocyclic ligands. Nucl Med Biol.
10 Hens M., Vaidyanathan G., Zhao X.G., Bigner D.D., Zalutsky M.R. (2010). Anti-EGFRvIII monoclonal antibody armed with 177Lu: in vivo comparison of macrocyclic and acyclic ligands. Nucl Med Biol.
11 Chopra, A., [125I]-Labeled monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
12 Chopra, A., 177Lu-Labeled 2-(4-isothiocyanatobenzyl)-6-methyldiethylene-triaminepentaacetic acid (1B4M-DTPA)) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
13 Chopra, A., [177Lu]-Labeled [(R)-2-amino-3-(4-isothiocyanatophenyl)propyl]-trans-(S,S)-cyclohexane-1,2-diamine-pentaacetic acid (CHX-A″-DTPA) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
14 Chopra, A., 177Lu-Labeled α-(5-isothiocyanato-2-methoxyphenyl)-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (MeO-DOTA) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.